# 2-(2-Nitro-1H-imidazol-1-yl)ethyl 2-[^18^F]fluoroacetate

Chemical name: | 2-(2-Nitro-1H-imidazol-1-yl)ethyl 2-[^18^F]fluoroacetate
Abbreviated name: | [^18^F]NEFT, [^18^F]8
Synonym:
Agent Category: | Compound
Target: | Hypoxic tissue
Target Category: | Hypoxia
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%202-Nitroimidazole)]

Hypoxia is found in a variety of solid tumors and leads to tumor progression and the resistance of tumors to chemotherapy and radiotherapy (1-3). Tumor oxygenation is heterogeneously distributed within human tumors (4). It would be beneficial to assess tumor oxygenation before and after therapy to provide an evaluation of tumor response to treatment and an insight into new therapeutic treatments (5). Tumor oxygenation is measured invasively using computerized, polarographic, oxygen-sensitive electrodes, which is regarded as the gold standard (6). Functional and non-invasive imaging of intratumoral hypoxia has been demonstrated to be feasible for the measurement of tumor oxygenation (7).

Chapman proposed the use of 2-nitroimidazoles for hypoxia imaging in 1979 (8). 2-Nitroimidazole compounds are postulated to undergo a reduction in hypoxic conditions, forming highly reactive oxygen radicals that subsequently bind covalently to macromolecules inside the cells (9). In normoxic conditions, the reduced molecule is rapidly reoxidized and transported from the cell. [^18^F]Fluoromisonidazole ([^18^F]FMISO (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=FMISO)) is the most widely used positron emission tomography (PET) tracer for imaging tumor hypoxia (7). However, it has slow clearance kinetics and high lipophilicity, resulting in substantial background signal in PET scans. [^18^F]Fluoroazomycinarabinofuranoside ([^18^F]FAZA (http://www.ncbi.nlm.nih.gov/books/NBK23282/)) is a 2-nitroimidazole with a sugar addition (10) and has been studied as a hypoxia-imaging agent, showing promising results in various tumor models in rats and mice (11, 12). Zha et al. (13) reported a new [^18^F]-labeled 2-nitroimidazole derivative, 2-(2-nitro-1H-imidazol-1-yl)ethyl 2-[^18^F]fluoroacetate ([^18^F]NEFT, which contains a hydrolyzable ester group for in vivo hypoxic tissue imaging.

### Related Resource Links:

- Chapters in MICAD (Hypoxia (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Hypoxia+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Hypoxia-inducible factor 1, alpha subunit (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3091))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Hypoxia (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=hypoxia%5BAll+Fields%5D))
- Clinical trials (Hypoxia imaging (http://www.clinicaltrials.gov/ct2/results?term=hypoxia+imaging))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NEFT%20and%20synthesis)]

[^18^F]NEFT was readily synthesized by ^18^F-fluorination of 2-(2-nitro-1H-imidazol-1-yl)ethyl2-bromoacetate ([^18^F]KF/18-crown-6/KHCO_3_, 10 min at 90°C) in dimethyl sulfoxide (13). [^18^F]NEFT was purified with solid-phase extraction. Overall yield was 9%–10% at the end of synthesis, with a radiochemical purity of >98%. Total synthesis time was ~60 min. The specific activity of [^18^F]NEFT was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NEFT%20and%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NEFT%20and%20rodentia)]

Ex vivo biodistribution studies of [^18^F]NEFT were performed in mice (n = 3) bearing EMT-6 tumors at 30 min after injection (13). The tumor accumulation was 2.45 ± 0.08% injected dose/gram (ID/g). The bone (6.29% ID/g) had the highest accumulation, followed by the lung (2.54% ID/g), blood (2.50% ID/g), heart (2.46% ID/g), kidney (2.38% ID/g), liver (2.23% ID/g), muscle (1.74% ID/g), spleen (1.71% ID/g), and brain (1.24% ID/g). The tumor/blood, tumor/liver, and tumor/muscle ratios were 0.98, 1.10, and 1.41, respectively. These ratios for [^18^F]FMISO were 0.91, 0.59, and 1.74, respectively. The authors suggested that enzymatic or chemical hydrolysis of [^18^F]NEFT would yield [^18^F]fluoroacetate. It is difficult to determine if the hypoxia or the trapping of [^18^F]fluoroacetate or both is more important for tumor accumulation. No blocking study was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NEFT%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NEFT%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=NEFT%20and%20humans)]

No publication is currently available.

## NIH Support

AG 022559-01

## References

1 Serkies K., Jassem J. (2005). Chemotherapy in the primary treatment of cervical carcinoma. Crit Rev Oncol Hematol.
2 Vaupel P., Mayer A. (2005). Hypoxia and anemia: effects on tumor biology and treatment resistance. Transfus Clin Biol.
3 Rajendran J.G., Krohn K.A. (2005). Imaging hypoxia and angiogenesis in tumors. Radiol Clin North Am.
4 Vaupel P., Harrison L. (2004). Tumor hypoxia: causative factors, compensatory mechanisms, and cellular response. Oncologist.
5 Dehdashti F., Grigsby P.W., Mintun M.A., Lewis J.S., Siegel B.A., Welch M.J. (2003). Assessing tumor hypoxia in cervical cancer by positron emission tomography with 60Cu-ATSM: relationship to therapeutic response-a preliminary report. Int J Radiat Oncol Biol Phys.
6 Raleigh J.A., Dewhirst M.W., Thrall D.E. (1996). Measuring Tumor Hypoxia. Semin Radiat Oncol.
7 Foo S.S., Abbott D.F., Lawrentschuk N., Scott A.M. (2004). Functional imaging of intratumoral hypoxia. Mol Imaging Biol.
8 Chapman J.D. (1979). Hypoxic sensitizers--implications for radiation therapy. N Engl J Med.
9 Chapman J.D., Baer K., Lee J. (1983). Characteristics of the metabolism-induced binding of misonidazole to hypoxic mammalian cells. Cancer Res.
10 Reischl G., Ehrlichmann W., Bieg C., Solbach C., Kumar P., Wiebe L.I., Machulla H.J. (2005). Preparation of the hypoxia imaging PET tracer [18F]FAZA: reaction parameters and automation. Appl Radiat Isot.
11 Piert M., Machulla H.J., Picchio M., Reischl G., Ziegler S., Kumar P., Wester H.J., Beck R., McEwan A.J., Wiebe L.I., Schwaiger M. (2005). Hypoxia-specific tumor imaging with 18F-fluoroazomycin arabinoside. J Nucl Med.
12 Sorger D., Patt M., Kumar P., Wiebe L.I., Barthel H., Seese A., Dannenberg C., Tannapfel A., Kluge R., Sabri O. (2003). [18F]Fluoroazomycinarabinofuranoside (18FAZA) and [18F]Fluoromisonidazole (18FMISO): a comparative study of their selective uptake in hypoxic cells and PET imaging in experimental rat tumors. Nucl Med Biol.
13 Zha Z., Zhu L., Liu Y., Du F., Gan H., Qiao J., Kung H.F. (2011). Synthesis and evaluation of two novel 2-nitroimidazole derivatives as potential PET radioligands for tumor imaging. Nucl Med Biol.